# NR-LU-10/streptavidin-copper 64-(1,4,7,10-tetraazacyclododecane-N,N′,N′′,N′′′-tetraacetic acid)-biotin

Chemical name: | NR-LU-10/streptavidin-copper 64-(1,4,7,10-tetraazacyclododecane-N,N′,N′′,N′′′-tetraacetic acid)-biotin
Abbreviated name: | NR-LU-10/SA-^64^Cu-DOTA-biotin
Synonym:
Agent Category: | Antibody
Target: | Epidermal cell adhesion molecules
Target Category: | Antibody–antigen recognition (with delivery of attached radionuclide)
Method of detection: | PET
Source of signal: | ^64^ Cu
Activation: | No
Studies: | - In vitro; - Rodents

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper-64-DOTA-biotin%22%5BSubstance%20Name%5D)]

Radiolabeled monoclonal antibodies (mAbs) have shown very promising results for cancer imaging. Nevertheless, because of their slow blood clearance, they do not localize in solid tumors in sufficient quantities to provide high contrast for positron emission tomography (PET) imaging. To overcome this problem, the innovative concept of antibody “pretargeting” can be used. This approach, first proposed by Goodwin et al. (1) 15 years ago, involves the administration of an unlabeled mAb construct that accumulates in tumors, followed by the administration of a radiolabeled molecule that binds rapidly with high affinity to the construct (2).

^64^Cu-DOTA-biotin can be labeled to high specificity with ^64^Cu and may be used as part of a mAb pretargeting approach, for example with pretreatment of the mAb-streptavidin (SA) conjugate NR-LU-10/SA (and the synthetic clearing agent biotin-GalNAc_16_) (3). The very rapid tumor uptake and blood clearance of ^64^Cu-DOTA-biotin make it possible to obtain a much higher PET imaging contrast than conventional imaging because of the increased permeability of the small, radiolabeled substrate.

The pretargeting strategy using the system NR-LU-10/SA -^64^Cu-DOTA-biotin takes advantage of the very high affinity between avidin (or streptavidin) and biotin (the dissociation constant K_d_ of the avidin/biotin complex is about 10^15^M); this characteristic has already been used in a wide range of in vitro and in vivo applications (4-6). Avidin and streptavidin have similar binding properties, although some of their chemical and physical properties are different. Streptavidin is often preferred to avidin, because of the slower blood clearance of the mAb conjugate (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SDZ%20215-811%22%5BSubstance%20Name%5D%20AND%20synthesis%5BAll%20Fields%5D)]

DOTA-biotin can be synthesized using the method from Lewis et al. (3). The labeling of DOTA-biotin with ^64^Cu can be performed using a modified protocol described previously in the literature (3, 8). Briefly, 0.114 μmol of DOTA-biotin (in 46.0 µl of 0.2 M ammonium acetate, pH 5.0) is added to 102 MBq (2.76 mCi) of ^64^Cu in 164 µl of 0.2 M ammonium acetate, pH 5.0, containing 1 mg/ml of gentisic acid). The reaction mixture is then incubated at 80°C for 1 h. The radiochemical purity of ^64^Cu-DOTA-biotin obtained by this method is between 95% and 100% (measured by thin-layer chromatography (TLC)).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper-64-DOTA-biotin%22%5BSubstance%20Name%5D%20AND%20%22in%20vitro%22%5BAll%20fields%5D)]

^64^Cu-DOTA-biotin can be assayed using a method described by Lewis et al. (3) and which involves mixing the radiolabeled compound with 4% streptavidin-agarose beads at room temperature. The amounts of ^64^Cu-DOTA-biotin that bound specifically to the immobilized streptavidin were found to be typically in the range of 98.4%-98.8%, whereas the immunoreactivity of ^64^Cu-DOTA-NR-LU-10 averaged 80%. In the experiments performed by Lewis et al. (3), direct labeling of DOTA-NR-LU-10 mAb, either through the binding of DOTA to the antibody or through the copper labeling procedure, appeared to decrease the immunoreactivity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper-64-DOTA-biotin%22%5BSubstance%20Name%5D%20AND%20%22rodentia%22%5BMeSH%5D)]

Biodistribution studies of NR-LU-10/SA-pretargeted ^64^Cu-DOTA-biotin in athymic nude mice bearing SW1222 human colorectal carcinoma xenografts were performed by Lewis et al. (3). Experimental data showed a very rapid accumulation of ^64^Cu-DOTA-biotin in tumor, reaching a tumor/blood ratio of 1.37 at 5 min after injection and a peak tumor uptake at 1 h with a tumor/blood ratio of 18.9. The blood and renal clearances of radioactivity were very rapid (from 20.8 % injected dose (ID)/g at 5 min to 3.40 % ID/g (P = 0.002) at 1 h for the kidneys). Other tissues that showed significant clearance (from 5 min to 48 h) were bone (P = 0.003) and the small intestine (P = 0.001).

Although the absolute tumor uptake of ^64^Cu-DOTA-NR-LU-10 was significantly higher than the ^64^Cu-DOTA-biotin, the pretargeting system exhibited much faster disappearance of radioactivity from the circulation (6 and 18 h were necessary for ^64^Cu-DOTA-NR-LU-10 levels (in % ID/g) to drop below the level of tumor uptake, and only 5 min was needed for the tumor/blood ratio of ^64^Cu-DOTA-biotin to exceed 1:1). Studies such as the one by Lewis et al. (3) showed that the antibody pretargeting strategy using NR-LU-10/SA and ^64^Cu-DOTA-biotin allows rapid clearance, superior tumor/normal tissue ratios, and whole-body radioactivity exposure from blood.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper-64-DOTA-biotin%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper-64-DOTA-biotin%22%5BSubstance%20Name%5D%20AND%20primates%20NOT%20humans)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22copper-64-DOTA-biotin%22%5BSubstance%20Name%5D%20AND%20%28%22humans%22%5BMeSH%20Terms%5D%20OR%20humans%5BText%20Word%5D%29)]

No publications of human studies involving the system NR-LU-10/SA-^64^Cu-DOTA-biotin

are currently available. Nevertheless, human data for DOTA-biotin labeled with other radionuclides, as well as clinical studies using the pretargeting system avidin-biotin, can be found in the literature (4, 9-11).

## References

1 Goodwin D, Meares C, Diamanti C, McCall M, Lai C, Torti F, McTigue M, Martin B. (1984). Use of specific antibody for rapid clearance of circulating blood background from radiolabeled tumor imaging proteins. Eur J Nucl Med.
2 Wu AM. (2001). Tools for pretargeted radioimmunotherapy. Cancer Biother Radiopharm.
3 Lewis MR, Wang M, Axworthy DB, Theodore LJ, Mallet RW, Fritzberg AR, Welch MJ, Anderson CJ. (2003). In vivo evaluation of pretargeted 64Cu for tumor imaging and therapy. J Nucl Med.
4 Paganelli G, Chinol M. (2003). Radioimmunotherapy: is avidin-biotin pretargeting the preferred choice among pretargeting methods?. Eur J Nucl Med Mol Imaging.
5 Goodwin DA, Meares CF. (2001). Advances in pretargeting biotechnology. Biotechnol Adv.
6 Hnatowich DJ, Virzi F, Rusckowski M. (1987). Investigations of avidin and biotin for imaging applications. J Nucl Med.
7 Sung C, van Osdol WW, Saga T, Neumann RD, Dedrick RL, Weinstein JN. (1994). Streptavidin distribution in metastatic tumors pretargeted with a biotinylated monoclonal antibody: theoretical and experimental pharmacokinetics. Cancer Res.
8 de Jong M, Bakker WH, Krenning EP, Breeman WA, van der Pluijm ME, Bernard BF, Visser TJ, Jermann E, Behe M, Powell P, Macke HR. (1997). Yttrium-90 and indium-111 labelling, receptor binding and biodistribution of [DOTA0,d-Phe1,Tyr3]octreotide, a promising somatostatin analogue for radionuclide therapy. Eur J Nucl Med.
9 Breitz HB, Fisher DR, Goris ML, Knox S, Ratliff B, Murtha AD, Weiden PL. (1999). Radiation absorbed dose estimation for 90Y-DOTA-biotin with pretargeted NR-LU-10/streptavidin. Cancer Biother Radiopharm.
10 Knox SJ, Goris ML, Tempero M, Weiden PL, Gentner L, Breitz H, Adams GP, Axworthy D, Gaffigan S, Bryan K, Fisher DR, Colcher D, Horak ID, Weiner LM. (2000). Phase II trial of yttrium-90-DOTA-biotin pretargeted by NR-LU-10 antibody/streptavidin in patients with metastatic colon cancer. Clin Cancer Res.
11 Gruaz-Guyon A, Raguin O, Barbet J. (2005). Recent advances in pretargeted radioimmunotherapy. Curr Med Chem.